# [^18^F]Fluoroethyl-recombinant human interlukin-1 receptor antagonist

Chemical name: | [^18^F]Fluoroethyl-recombinant human interlukin-1 receptor antagonist
Abbreviated name: | [^18^F]IL-1ra
Synonym: | [^18^F]IL-1RN, [^18^F]FE-rhIL-1ra
Agent category: | Polypeptide
Target: | IL-1 receptors (IL-1R1 and IL-1R2)
Target category: | Receptor
Method of detection: | Positron emission tomography (PET)
Source of signal/contrast: | ^18^F
Activation: | No
Studies: | - In vitro; - Rodents | Click on protein (http://www.ncbi.nlm.nih.gov/protein/CAA36262.1), nucleotide (http://www.ncbi.nlm.nih.gov/nuccore/NM_173842.2) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/gene/3557) for more information about Interlukin-1 receptor antagonist (IL-1ra).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=IL-1ra%20AND%20PET)]

The interleukin-1 family consists of two proinflammatory cytokines, IL-1α and IL-1β, which bind to two IL-1 receptors (IL-1R1 and IL-1R2), and an IL-1R antagonist (IL-1ra), which is mainly produced by activated macrophages and tissue macrophages (1). IL-1α and IL-1β are important mediators of the inflammatory response and hematopoiesis, and they are involved in a variety of cellular activities, including cell proliferation, differentiation, and apoptosis. IL-1 is involved in chronic inflammatory diseases and in neuropathological conditions (2, 3). The balancing act of IL-1 and IL-1ra plays an important role in regulation of inflammation and immune responses (4). IL-1ra has been shown to be effective as an anti-inflammatory treatment in several chronic inflammatory diseases and stroke (5, 6). A human recombinant, non-glycosylated form of the human IL-1ra (rhIL-1ra, Anakinra (http://google2.fda.gov/search?q=anakinra&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&filter=1&requiredfields=-archive%3AYes)) has been approved by the United States Food and Drug Administration for the treatment of rheumatoid arthritis (7). Cawthorne et al. (8) used positron emission tomography (PET) imaging to evaluate the biodistribution of [^18^F]fluoroethyl-recombinant human interleukin-1 receptor antagonist ([^18^F]IL-1ra) in rats.

### Related Resource Links:

- Chapters in MICAD (IL-1 (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=books&Cmd=DetailsSearch&Term=IL-1%20Y%20%5BAll+Fields%5D+AND+micad%5Bbook%5D))
- Gene information in NCBI (IL-1á (http://www.ncbi.nlm.nih.gov/gene/3552), IL-1â (http://www.ncbi.nlm.nih.gov/gene/3553) IL-1R1 (http://www.ncbi.nlm.nih.gov/gene/3554), IL-1R2 (http://www.ncbi.nlm.nih.gov/gene/7850), IL-1ra (http://www.ncbi.nlm.nih.gov/gene/3557))
- Articles in Online Mendelian Inheritance in Man (OMIM) (IL-1á (http://omim.org/entry/147760), IL-1â (http://omim.org/entry/147720), IL-1R1 (http://omim.org/entry/147810), IL-1R2 (http://omim.org/entry/147811), IL-1ra (http://omim.org/entry/147679))
- Clinical trials (IL-1 (http://www.clinicaltrials.gov/ct2/results?term=IL-1&Search=Search), IL-1ra (http://www.clinicaltrials.gov/ct2/results?term=il-1ra&Search=Search), Anakinra (http://www.clinicaltrials.gov/ct2/results?term=anakinra))
- Drug information in FDA (Anakinra (http://google2.fda.gov/search?q=anakinra&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&filter=1&requiredfields=-archive%3AYes))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=IL-1ra%20AND%20PET%20and%20synthesis)]

The radiosynthesis of [^18^F]IL-1ra, reported by Prenant et al. (9), involved reductive amination on Lys moieties of rhIL-1ra with [^18^F]fluoroacetaldehyde for 45 min at 38°C (pH 6). [^18^F]IL-1ra was purified on a desalting column, with a specific activity of 0.81–4.9 MBq/nmol (0.022–0.13 mCi/nmol) at the end of synthesis. The radiochemical purity was >95%, and the total synthesis time was ~60 min.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=IL-1ra%20AND%20PET%20and%20in%20vitro)]

Prenant et al. (9) performed in vitro autoradiography on rat brain sections using [^18^F]IL-1ra. Excess unlabeled IL-1ra reduced radioactivity accumulation in the brain sections. However, the specific binding of [^18^F]IL-1ra to IL-1 receptors was only 24%–29% of total binding.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=IL-1ra%20AND%20PET%20and%20rodentia)]

Cawthorne et al. (8) performed ex vivo biodistribution (n = 3–4/group) and dynamic whole-body PET imaging (n = 6) studies in normal rats after injection of 12.4–30.5 MBq [^18^F]IL-1ra. The organs studied were the brain, liver, lung, and kidney, and they demonstrated a rapid distribution and elimination of radioactivity. The kidneys showed an initial accumulation of ~3% injected dose (ID)/cm^3^ at 2 min, a rapid increase to 10% ID/cm^3^ at 10 min, and a slow decline to 2% ID/cm^3^ at 90–120 min. The lungs and liver exhibited an initial accumulation of 1.2% and 1.0% ID/cm^3^ at 2 min and a rapid decline to a plateau of 0.3% ID/cm^3^ at 20–120 min. The accumulation in the brain was lower than the peripheral organs, with 0.11% ID/cm^3^ at 20 min and 0.10% ID/cm^3^ at 120 min. Ex vivo data (20, 60, and 120 min) showed that the relative distribution between organs was consistent with the PET imaging data (brain<< lungs < liver << kidneys). [^18^F]IL-1ra remained >98% intact in the blood at 1, 5, and 10 min after injection, whereas blood [^18^F]IL-1ra remained 65%, 15%, and 6% intact at 20, 60, and 120 min, respectively. [^18^F]IL-1ra was degraded into smaller metabolites.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=IL-1ra%20AND%20PET%20and%20%28dog%20or%20pig%20or%20sheep%20or%20rabbit%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=IL-1ra%20AND%20PET%20and%20%28primate%20not%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=IL-1ra%20AND%20PET%20and%20human)]

No publication is currently available.

## References

1 Dinarello C.A. (1996). Biologic basis for interleukin-1 in disease. Blood.
2 McColl B.W., Allan S.M., Rothwell N.J. (2009). Systemic infection, inflammation and acute ischemic stroke. Neuroscience.
3 Simi A., Tsakiri N., Wang P., Rothwell N.J. (2007). Interleukin-1 and inflammatory neurodegeneration. Biochem Soc Trans.
4 Dinarello C.A., Simon A., van der Meer J.W. (2012). Treating inflammation by blocking interleukin-1 in a broad spectrum of diseases. Nat Rev Drug Discov.
5 Neven B., Marvillet I., Terrada C., Ferster A., Boddaert N., Couloignier V., Pinto G., Pagnier A., Bodemer C., Bodaghi B., Tardieu M., Prieur A.M., Quartier P. (2010). Long-term efficacy of the interleukin-1 receptor antagonist anakinra in ten patients with neonatal-onset multisystem inflammatory disease/chronic infantile neurologic, cutaneous, articular syndrome. Arthritis Rheum.
6 Emsley H.C., Smith C.J., Georgiou R.F., Vail A., Hopkins S.J., Rothwell N.J., Tyrrell P.J. (2005). A randomised phase II study of interleukin-1 receptor antagonist in acute stroke patients. J Neurol Neurosurg Psychiatry.
7 Thompson R.C., Dripps D.J., Eisenberg S.P. (1992). Interleukin-1 receptor antagonist (IL-1ra) as a probe and as a treatment for IL-1 mediated disease. Int J Immunopharmacol.
8 Cawthorne C., Prenant C., Smigova A., Julyan P., Maroy R., Herholz K., Rothwell N., Boutin H. (2011). Biodistribution, pharmacokinetics and metabolism of interleukin-1 receptor antagonist (IL-1RA) using [(1)(8)F]-IL1RA and PET imaging in rats. Br J Pharmacol.
9 Prenant C., Cawthorne C., Fairclough M., Rothwell N., Boutin H. (2010). Radiolabeling with fluorine-18 of a protein, interleukin-1 receptor antagonist. Appl Radiat Isot.